# ^131^I-Labeled arginine-arginine-leucine (RRL)-containing cyclic peptide (YCGGRRLGGC) for imaging prostate carcinoma

Chemical name: | 131I-labeled arginine-arginine-leucine (RRL)-containing cyclic peptide (YCGGRRLGGC) for imaging prostate carcinoma
Abbreviated name: | ^131^I-Labeled RRL peptide
Synonym: | WT1040
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=integrins+and+targeting)]

Integrins are transmembrane glycoproteins with two noncovalently bound α and β subunits. The two subunits mediate cell–cell and cell–extracellular matrix (ECM) interactions, and they act downstream of several primary signaling events that lead to angiogenesis (1-4). Integrins comprise a large family of cell adhesion molecules, and integrin α_v_β_3_ appears to be the most attractive member for angiogenesis-targeted imaging and therapy because of its critical involvement in tumor angiogenesis, development, and metastasis. Integrin α_v_β_3_ is minimally expressed in normal blood vessels but is significantly upregulated in newly sprouting vasculature in tumors (2, 4, 5).

A significant effort has been made to generate various imaging agents targeting integrin α_v_β_3_ (1, 4, 6-9). Generally, these agents can be categorized as antibodies, peptides, small-molecule peptidomimetics, and targeted nanoparticles. Vitaxin is the representative of monoclonal antibodies against integrin α_v_β_3_. Vitaxin is a humanized antibody composed of human IgG-1, kappa, and the complement domain regions of the murine antibody LM 609. Regardless of its efficacy in inhibiting angiogenesis, imaging with ^99m^Tc-labeled Vitaxin failed to show the tumor angiogenesis in the clinical settings because of its poor stability and rapid plasma clearance with low doses (10). Interestingly, Gutheil et al. have reported that second-generation Vitaxin-2–conjugated, gadolinium-encapsulated nanoparticles could provide enhanced and detailed imaging of rabbit carcinomas and imaging of angiogenic “hot spots” that are not seen with standard magnetic resonance imaging (11). The major limitations of monoclonal antibodies include large molecular size, low production yield, incomplete tumor penetration, and immunogenicity to host.

Numerous small peptides have been identified to specifically interact with tumor neovasculature, including arginine-glycine-aspartic acid (RGD), asparagine-glycine-arginine, histidine-tryptophan-glycine-phenylalanine, and arginine-arginine-leucine (RRL) (7, 12-16). RGD tripeptide sequence is known as a cell recognition site for adhesive proteins present in the ECM and in blood. Integrin α_v_β_3_ binds ECM proteins through the exposed RGD tripeptide in their ligands. Both linear and cyclic RGD peptide agents have been proven to be useful in imaging tumor neovasculature. In general, linear peptides are broken down rapidly in vivo and occupy a wide range of conformations, resulting in low binding affinity and less specific accumulation within tumors. Short cyclic peptides are superior to linear peptides for their pharmacokinetics due to the fact that they are trapped in the active conformation and are more resistant to proteolysis. The pharmacokinetic behaviors of RGD peptides can be further improved with introduction of sugar moiety, the dimeric format of RGD peptides, or coupling with 1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid or polyethylene glycol (12, 13, 15). However, RGD peptides are less selective (binding with 8 of the 24 integrins), and their binding affinities are relatively low (50% inhibition concentration (IC_50_), 20–70 nmol) compared to antibodies. A series of non-peptide α_v_β_3_ chemical antagonists including IntegriSense (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html) (IC_50_, 4.1 nmol; binding with α_v_β_3_/α_v_β_5_ only) have recently been shown to accumulate specifically in α_v_β_3_/α_v_β_5_-expressing tumors with high affinity and specificity (14). More recently, several classes of peptidomimetic integrin α_v_β_3_ antagonists have been reported (6, 17). These peptidomimetic antagonists consist of a rigid core scaffold bearing basic and acidic groups that mimic the guanidine and carboxylate groups of the RGD sequence. Additionally, ligand array of integrin antagonists on nanoparticles has been proven to be a viable strategy to target vascular surface receptors on endothelial cells. Imaging studies are in progress with these new strategies (6).

Nevertheless, small peptides have distinct advantages such as easy synthesis, less immunogenicity, and rapid plasma clearance. In addition to RGD, the tripeptide sequence RRL has been investigated to generate imaging agents (16, 18). RRL is a tumor endothelial cell–specific binding peptide previously identified by Brown et al. using an in vitro bacterial peptide display library panned against tumor cells (19). Weller et al. have shown that the microbubble-linked RRL peptide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=RRL-MB) preferentially adheres to tumor versus normal vasculature, and this selective adherence can be detected with ultrasound (18). Yu et al. studied the radionuclide-labeled RRL peptide (designated WT1040) for tumor imaging and demonstrated that the ^131^I-labeled RRL peptide allowed non-invasive visualization of tumors (16).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=integrin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Integrin-related articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=integrins)
- Integrin á_v_â_3_-related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=Integrin+%CE%B1v%CE%B23)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=arginine-arginine-leucine+peptide)]

The RRL peptide (Tyr-Cys-Gly-Gly-Arg-Arg-Leu-Gly-Gly-Cys-NH_2_) and the control peptide (Tyr-Cys-Gly-Gly-Gly-Gly-Gly-Gly-Gly-Cys-NH_2_) were synthesized with the solid-phase peptide synthesis method, and the disulfide bonds between cysteines on each peptide were formed to maintain the cyclic structure. The cysteine at the C-terminal of RRL and control peptides was amidated to protect the peptides from rapid biodegradation. Radioiodination of the peptides was performed with the chloramine-T method (16). The best RRL peptide/chloramine-T weight ratio was 1:1.8. When the ratio differed from this value, the radiolabeling yield decreased. When the reaction time was 1, 3, 5, and 10 min, the radiolabeling yield reached 60, 62, 65, and 65%, respectively. When the input of peptide was 10, 30, and 50 µg, the radiolabeling yield reached 40.3, 49.7, and 60%, respectively. The radiochemical purity of ^131^I-labeled RRL peptide was >95%. The molecular weight was 1040.2 before oxidation and 1038.2 after oxidation. The specific activity was not reported. After incubation at 37°C with human blood serum, the radiochemical purities of ^131^I-labeled RRL peptide were 96.1 ± 0.40, 95.7 ± 0.35, 95.5 ± 1.38, 94.8 ± 0.35, and 90.3 ± 0.63% at 1, 2, 4, 8, and 24 h, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19920196?ordinalpos=&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.SmartSearch&log$=citationsensor)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=arginine-arginine-leucine+peptide)]

Yu et al. analyzed the biodistribution of ^131^I-labeled RRL and compared it with that of control peptide in 4–6-week-old male BALB/c nude mice bearing PC3 human prostate carcinoma xenografts (16). The tissue uptake was measured at 1, 6, and 24 h after injection (n = 3 mice/group). Highest uptake for both radiotracers was observed in the kidney, liver, and intestine. There was no difference for the tumor uptake between ^131^I-labeled RRL and control peptides at 1 h after injection (P > 0.05), but the ^131^I-labeled RRL signal decreased more slowly over time in tumors (74% from 6 to 24 h) than in the kidneys (86%), muscle (90%), and other organs. Radiolabeled RRL peptide accumulated in the tumor at ~2.52% and ~0.65% injected dose per gram of tissue (ID/g) at 6 h and 24 h after injection, respectively, higher than in other organs (P < 0.05), whereas this value for ^131^I-labeled control peptide was only 0.73% and 0.06% ID/g (both P < 0.05) at 6 h and 24 h, respectively. The tumor/tissue ratios (with the exception of the lung) increased with time for RRL peptide but did not increase for the control peptide. At 1, 6, and 24 h after injection, the tumor/blood ratios were 0.32, 1.12, and 1.30 for RRL peptide and 0.30, 0.37, and 0.22 for control peptide, respectively, and the tumor/muscle ratios were 1.40, 3.94, and 9.08 for RRL peptide and 1.98, 2.89, and 1.78 for control peptide, respectively. No blocking studies were carried out.

Single-photon emission computed tomography of mice bearing human prostate carcinoma after injection of ^131^I-labeled RRL peptide showed high radioactivity in the thyroid, abdomen, and bladder at 1 h and in the thyroid and abdomen at 3 h, and showed low radioactivity in the tumor at both 1 h and 3 h. At 24 h after injection, high radioactivity was observed in the tumor, and the surrounding background was very low. The thyroid was no longer detected (16).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lim E.H., Danthi N., Bednarski M., Li K.C. (2005). A review: Integrin alphavbeta3-targeted molecular imaging and therapy in angiogenesis. Nanomedicine.
2 Desgrosellier J.S., Cheresh D.A. (2010). Integrins in cancer: biological implications and therapeutic opportunities. Nat Rev Cancer.
3 Caswell P.T., Vadrevu S., Norman J.C. (2009). Integrins: masters and slaves of endocytic transport. Nat Rev Mol Cell Biol.
4 Beer A.J., Schwaiger M. (2008). Imaging of integrin alphavbeta3 expression. Cancer Metastasis Rev.
5 Schnell O., Krebs B., Wagner E., Romagna A., Beer A.J., Grau S.J., Thon N., Goetz C., Kretzschmar H.A., Tonn J.C., Goldbrunner R.H. (2008). Expression of integrin alphavbeta3 in gliomas correlates with tumor grade and is not restricted to tumor vasculature. Brain Pathol.
6 Blankenberg F.G., Mari C., Strauss H.W. (2002). Development of radiocontrast agents for vascular imaging: progress to date. Am J Cardiovasc Drugs.
7 Dijkgraaf I., Boerman O.C. (2009). Radionuclide imaging of tumor angiogenesis. Cancer Biother Radiopharm.
8 Ruegg C., Alghisi G.C. (2010). Vascular integrins: therapeutic and imaging targets of tumor angiogenesis. Recent Results Cancer Res.
9 Stollman T.H., Ruers T.J., Oyen W.J., Boerman O.C. (2009). New targeted probes for radioimaging of angiogenesis. Methods.
10 Posey J.A., Khazaeli M.B., DelGrosso A., Saleh M.N., Lin C.Y., Huse W., LoBuglio A.F. (2001). A pilot trial of Vitaxin, a humanized anti-vitronectin receptor (anti alpha v beta 3) antibody in patients with metastatic cancer. Cancer Biother Radiopharm.
11 Gutheil J.C., Campbell T.N., Pierce P.R., Watkins J.D., Huse W.D., Bodkin D.J., Cheresh D.A. (2000). Targeted antiangiogenic therapy for cancer using Vitaxin: a humanized monoclonal antibody to the integrin alphavbeta3. Clin Cancer Res.
12 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
13 Dijkgraaf I., Kruijtzer J.A., Liu S., Soede A.C., Oyen W.J., Corstens F.H., Liskamp R.M., Boerman O.C. (2007). Improved targeting of the alpha(v)beta (3) integrin by multimerisation of RGD peptides. Eur J Nucl Med Mol Imaging.
14 Kossodo, S., M. Pickarski, S.A. Lin, A. Gleason, R. Gaspar, C. Buono, G. Ho, A. Blusztajn, G. Cuneo, J. Zhang, J. Jensen, R. Hargreaves, P. Coleman, G. Hartman, M. Rajopadhye, L.T. Duong, C. Sur, W. Yared, J. Peterson, and B. Bednar, Dual In Vivo Quantification of Integrin-targeted and Protease-activated Agents in Cancer Using Fluorescence Molecular Tomography (FMT). Mol Imaging Biol, 2009
15 Liu S. (2006). Radiolabeled multimeric cyclic RGD peptides as integrin alphavbeta3 targeted radiotracers for tumor imaging. Mol Pharm.
16 Yu M., Zhou H., Liu X., Huo Y., Zhu Y., Chen Y. (2010). Study on biodistribution and imaging of radioiodinated arginine-arginine-leucine peptide in nude mice bearing human prostate carcinoma. Ann Nucl Med.
17 Sillerud L.O., Larson R.S. (2005). Design and structure of peptide and peptidomimetic antagonists of protein-protein interaction. Curr Protein Pept Sci.
18 Weller G.E., Villanueva F.S., Tom E.M., Wagner W.R. (2005). Targeted ultrasound contrast agents: in vitro assessment of endothelial dysfunction and multi-targeting to ICAM-1 and sialyl Lewisx. Biotechnol Bioeng.
19 Brown C.K., Modzelewski R.A., Johnson C.S., Wong M.K. (2000). A novel approach for the identification of unique tumor vasculature binding peptides using an E. coli peptide display library. Ann Surg Oncol.